# ^111^In-Labeled panitumumab, a fully human monoclonal antibody directed against the extracellular domain III of the epidermal growth factor receptor

Chemical name: | ^111^In-Labeled panitumumab, a fully human monoclonal antibody directed against the extracellular domain III of the epidermal growth factor receptor
Abbreviated name: | [^111^In]-Panitumumab
Synonym:
Agent Category: | Antibody
Target: | Epidermal growth factor receptor (EGFR) extracellular domain III
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=panitumumab&cmd=DetailsSearch)]

Panitumumab (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=e0fa4bca-f245-4d92-ae29-b0c630a315c2) is a fully human anti-epidermal factor receptor (EGFR) monoclonal antibody (mAb) that has been approved by the United States Food and Drug Administration (FDA) for the treatment of metastatic colorectal cancers (http://cancer.gov/cancertopics/wyntk/colon-and-rectal) that express the EGFR and are unresponsive to chemotherapy (1). This mAb has a very high affinity for the extracellular domain III of the EGFR. The general characteristics of panitumumab have been described by Argiles et al. (2), and its mode of action has been illustrated by Dubois and Cohen (1). The fully human mAb has been reported to be well tolerated by individuals, slows disease progression, and improves the progression-free survival of patients (3). Therefore, [^111^In]-labeled panitumumab ([^111^In]-panitumumab) was evaluated for the noninvasive detection of EGFR-positive tumors in an effort to screen for patients who would benefit from radioimmunotherapy with this mAb after it was labeled with a suitable radionuclide (3). The ^111^In-labeled mAb was studied in vitro, and the biodistribution of [^111^In]-panitumumab was investigated in athymic mice bearing xenograft tumors generated with A431 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2592&Template=cellBiology), HT-29 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-38&Template=cellBiology), LS-174T (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CL-188&Template=cellBiology), SHAW (obtained from the National Cancer Institute), and SKOV-3 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-77&Template=cellBiology) cell lines, respectively (3). In addition, gamma scintigraphic images were acquired from mice bearing xenograft tumors to confirm noninvasive visualization of the lesions.

### Related Resource Links

Panitumumab-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books?term=Panitumumab%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D&cmd=DetailsSearch)

EGFR-related chapters (http://www.ncbi.nlm.nih.gov/books/?term=EGFR+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) in MICAD

EGFR (http://pid.nci.nih.gov/search/intermediate_landing.shtml?molecule=EGFR)(in Pathways Interaction Database)

EGFR in Online Mendelian Inheritance in Man Database (OMIM (http://omim.org/entry/131550))

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Panitumumab) with panitumumab

Other anti-EGFR antibodies approved for clinical use by the FDA (cetuximab (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=8bc6397e-4bd8-4d37-a007-a327e4da34d9), trastuzumab (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=492dbdb2-077e-4064-bff3-372d6af0a7a2))

EGFR tyrosine kinase inhibitors [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=EGFR%20tyrosine%20kinase%20inhibitors&cmd=DetailsSearch)]

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5Dpanitumumab%20synthesis&cmd=DetailsSearch)]

The source of panitumumab was not disclosed, and the mAb was conjugated with diethylenetriamine pentaacetic acid (CHX-A''-DTPA), a bifunctional chelating agent, for labeling with ^111^In (3). The CHX-A''-DTPA:mAb ratio was reported to be 1.6. The radiochemical yield of the labeling reaction was 68.7 ± 12.3%, and the specific activity of the labeled mAb was 721.5 ± 329.3 MBq/66.6 nmol (19.5 ± 8.9 mCi/66.6 nmol). The radiochemical purity, stability, and formulation of the final [^111^In]-panitumumab preparation was not reported (3).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5Dpanitumumab%20in%20vitro%20studies&cmd=DetailsSearch)]

A flow cytometric assay showed that the A431, HT-29, LS-174T, SHAW, and SKOV-3 cells expressed the EGFR (3). Using a competition radioimmunoassay (RIA) with [^125^I]-panitumumab as the ligand, the immunoreactivity of the panitumumab-CHX-A''-DTPA conjugate was shown to be similar to that of the native mAb (3). Exposure of A431 cells to [^111^In]-panitumumab showed that 74 ± 7.5% of the total radioactivity added to the assay was bound to the cells (3). Addition of 66.6 nmol nonradioactive panitumumab to the assay mixture resulted in only 4.0 ± 0.9% of radioactivity binding to the cells. This indicated that [^111^In]-panitumumab had a binding specificity for the EGFR.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5Dpanitumumab%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^111^In]-panitumumab was investigated in normal athymic mice (without tumors) and athymic mice bearing A431 cell tumors, as described by Ray et al. (3). The animals were injected with ~0.28 MBq (~7.5 μCi) [^111^In]-panitumumab through the tail vein, and the rodents (n = 5 mice/time point) were euthanized at 24, 48, 72, 96, and 168 h postinjection (p.i.) to harvest the major organs, including the tumors, to determine the uptake of radioactivity in the different tissues. Results obtained from this study were presented as percent of injected dose per milliliter (% ID/mL). In the normal mice, maximum radioactivity was observed in the salivary glands at 96 h p.i. (~15.0% ID/mL), followed by the liver at 24 h p.i. (~8.0% ID/mL), the gall bladder at 72 h p.i. (~7.5% ID/mL), and the lungs at 48 h p.i. (~7.0% ID/mL). The mice with tumors showed maximum accumulation of radioactivity in the tumor at 96 h p.i. (~17.0% ID/mL), followed by the brain at 24 h p.i. (~7.5% ID/mL), the salivary glands at 48 h p.i. (~6.5% ID/mL), and the kidneys at 24 h p.i. (~6.0% ID/mL). All other organs from the mice bearing tumors showed uptake values of <5.0% ID/mL at the various time points. No blocking studies were reported.

The biodistribution of [^111^In]-panitumumab was also studied in athymic mice bearing subcutaneous xenograft tumors (n = 5 animals/time point per tumor type) of HT-29 cells, LS-174T cells, SHAW cells, and SKOV-3 cells, respectively (3). Maximum uptake of label was observed in the tumor tissues of all the tumor models. Among the tumor types, the LS-174T cell human colon carcinoma xenograft tumors showed the highest accumulation of radioactivity (44.08 ± 9.53% ID/mL at 48 h p.i.). No blocking studies were reported.

For gamma scintigraphy, mice bearing xenograft tumors derived from the various cell lines were injected with 3–3.7 MBq (80–100 μCi) [^111^In]-panitumumab, and images were acquired from the animals at various time points from 24 h p.i. to 168 h p.i (3). The images showed that the tumors were clearly visible within 48 h p.i. Among the tumors, the LS-174T cell lesions remained visible for up to 168 h p.i (3). From the images it was apparent that high amounts of the label were present in the blood, heart, lung, and liver at 24 h p.i., and the radioactivity subsequently cleared from these tissues over the next week. No blocking studies were reported.

Results obtained from the various studies indicated that [^111^In]-panitumumab was a suitable tracer for the detection of tumors that express the EGFR in rodents (3).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5Dpanitumumab%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5Dpanitumumab%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5Dpanitumumab%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Work presented in this chapter was supported by the Intramural Research Program of the National Institutes of Health, National Cancer Institute, and the Center for Cancer Research.

## References

1 Dubois E.A., Cohen A.F. (2009). Panitumumab. Br J Clin Pharmacol.
2 Argiles G., Dienstmann R., Elez E., Tabernero J. (2012). Panitumumab: a summary of clinical development in colorectal cancer and future directions. Future Oncol.
3 Ray G.L., Baidoo K.E., Wong K.J., Williams M., Garmestani K., Brechbiel M.W., Milenic D.E. (2009). Preclinical evaluation of a monoclonal antibody targeting the epidermal growth factor receptor as a radioimmunodiagnostic and radioimmunotherapeutic agent. Br J Pharmacol.